# Avidin-coated baculoviral vectors-biotinylated ultra-small superparamagnetic iron oxide nanoparticles

Chemical name: | Avidin-coated baculoviral vectors-biotinylated ultra-small superparamagnetic iron oxide nanoparticles
Abbreviated name: | Baavi-bUSPIO
Synonym:
Agent category: | Protein, nanoparticle (virus)
Target: | Other
Target category: | Other
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxides
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=baavi +USPIO)]

Gene therapy delivers a functional gene into a target cell to restore the physiological levels of the deficient gene (1, 2). This therapeutic methodology has been used in the clinic to treat diseases and cancers induced by genetic disorders (3). For example, a cytotoxic gene can destroy a specific type of cancer cell without excessive damage to normal tissue (4). Because viruses are inherently capable of packaging nucleic acids and delivering them to susceptible cells with high efficiency, they become a preferred system for natural gene therapy delivery (5). Viral vectors can be engineered with a gene expression cassette or converted to a targeted vector. Both methods allow delivery of the gene of interest (transgene) to the desired cells or tissues (3). As a gene therapy vector, the viruses need to meet three criteria: safety, high transfer efficiency, and reliable transgene expression. Assessment of the development of viral vectors in vivo becomes an important step in the implementation of gene therapy in the clinic. With its inherent high spatial resolution, magnetic resonance imaging (MRI) can be effectively used to examine the pharmacokinetics and development of viral vectors in vivo, especially their adsorption, distribution, biotransformation, and excretion.

Baculoviruses (BV) are a family of rod-shaped viruses with a circular, double-stranded genome ranging from 80 to 180 kbp that can encode ~100–200 proteins (6). BV mainly replicates in insect cells, not in mammalian cells, through the function of a glycoprotein gp64 (512 amino acids) located on the viral envelop (7). BV can efficiently mediate gene transfer in mammalian cells in the presence of active mammalian cell promoters such as the cytomegalovirus promoter. The inherent inability of BV to replicate in mammalian cells makes it an attractive candidate for gene therapy (7) and for protein expressions such as ion channels, G-protein–coupled receptors, nuclear receptors, and transporters (5). As a gene delivery vector, BV has several unique features, including extremely high levels of gene expression and accessibility and an excellent biosafety profile (5). A BV with avidin is a recombinant BV that has avidin inserted into its native envelope glycoprotein gp64 (8). The presence of avidin on the surface of the BV provides a versatile platform, the avidin displaying BV (Baavi), for binding a variety of biotinylated molecules, including imaging probes (9). The insertion of avidin also increases the transduction efficiency of BV by 5–26-fold (8).

Complexation of Baavi with biotinylated ultra-small superparamagnetic iron oxide nanoparticles (bUSPIO) forms an agent (Baavi-bUSPIO) used for MRI imaging of recombinant BV (9). The USPIOs contain an icosahedral core of superparamagnetic crystalline Fe_3_O_4_ (magnetite) (10). They possess a high magnetic susceptibility that results in a significant induced magnetization inside a magnetic field. This creates microscopic field gradients that diphase nearby protons and cause a shortening of T_2_ relaxation times (11). With a 50-nm USPIO and a virus of approximately 25 nm × 200 nm, each bUSPIO binds ~1–2 viruses. The Baavi includes a LacZ transgene, which is a gene for encoding of a common enzymatic reporter protein β-galactosidase (β-gal) (12). The presence of β-gal allows for quantitative measurement of transduction efficiency of Baavi-bUSPIO in vitro and/or histological evaluation of Baavi-bUSPIO in targeted tissues ex vivo.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(baavi +USPIO)+AND+synthesis%0D%0A)]

Baavi-bUSPIO was obtained by conjugation of Baavi with bUSPIO (9). Baavi was prepared in several steps (8). First, a β-gal (LacZ) cassette was cloned into a PυuII site of modified pFastBac1 donor vector under a cytomegalovirus (CMV) promoter to serve as the Baavi backbone. The SrfI site of the produced plasmid (BVlacZ) was ligated to a linker with a StuI site. Second, the avidin-gp64 sequence was included in the BVlacZ under the control of the polyhedrin promoter. The resulting 408-bp fragment was digested and subcloned into the PstI site of a pBACSurf-1 vector. Third, the EcoRV/SnaBI fragment (2,173 bp) containing the avidin-gp64 cassette was cloned between the StuI sites of BVlacZ to produce the Baavi donor plasmid. Finally, the recombinant Baavi viruses were generated using the standard Bac-to-Bac method. Successful avidin-gp64 fusion protein expression was confirmed with immunoblot assays. At the same time, bUSPIOs were obtained by coating 50-nm USPIOs with d-biotin in the presence of O-benzotriazole N,N,N’,N’-tetramethyl-uronium-hexafluorophosphate as a coupling agent (9). Baavi (2.5 × 10^10^ infective particle/ml) was mixed with bUSPIOs at a ratio of ~100 spheres per infective virus particle and incubated overnight at 4ºC to produce Baavi-bUSPIO.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(baavi + USPIO)+AND+%22in+vitro%22)]

The complex of Baavi-bUSPIO was examined with atomic force microscopy (9). Approximately 1–2 Baavi particles (200–300 nm long and 24–27 nm wide) were found per bUSPIO (42 ± 7 nm). The cytotoxicity of Baavi-bUSPIO was assessed with 3-[4,5-dimethylthiazol-2-yl]-2,5-diphenyltetrazolium bromide (MTT) viability assay (no data were reported) (9). The transduction efficiency of Baavi-bUSPIO was assessed in HepG2 cells (9). The cells were stained with X-gal to visualize β-gal–expressing cells 24 hr after incubation with Baavi-bUSPIO. The presence of Baavi-bUSPIO appeared to increase the transduction efficiency and transgene expression level.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(baavi +USPIO) +AND++rodentia)]

Raty et al. studied the distribution of Baavi-bUSPIO in rats with MRI at 4.7 T (9). Doses of Baavi-bUSPIO were injected intraventrically into rat brains, and MRI images were collected 2 h after injection and 1, 3, 6 days (n = 7), and 14 days (n = 2). A 10-μl solution that contained bUSPIO in 500 ng Fe and 2.5 × 10^8^ infective Baavi was injected into the right ventricle. The Baavi was expected to deliver the cargo bUSPIO to choroid plexus cells. MRI images revealed that Baavi-bUSPIO was located in the ipsilateral ventricle of rat brains as soon as 2 h after injection, and the signal remained detectable for 2 weeks. In comparison, injection of an equal amount of bUSPIO did not generate similar contrast. Two types of histological staining were used to further confirm the distribution of Baavi-bUSPIO (9). Rats were euthanized at different time points after MRI sessions. Iron content was examined with diaminobenzene-enhanced Prussian Blue staining. Consistent staining was found in the cuboid epithelial cells of the choroid plexus in tissue sections from the ipsilateral side, whereas the rest of the brain remained unstained. The expression of the nuclear-targeted LacZ transgene in the cryosectioned brain was examined with β-gal staining. Rats injected with Baavi-bUSPIO exhibited a large number of positively stained cells in the choroid plexus, which was comparable to those injected with wild-type Baavi that contained LacZ. These stained tests confirmed the MRI observations.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( baavi+USPIO) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(baavi + USPIO) +AND+human)]

No publication is currently available.

## References

1 Glover D.J., Lipps H.J., Jans D.A. (2005). Towards safe, non-viral therapeutic gene expression in humans. Nat Rev Genet.
2 Kootstra N.A., Verma I.M. (2003). Gene therapy with viral vectors. Annu Rev Pharmacol Toxicol.
3 Peng K.W. (1999). Strategies for targeting therapeutic gene delivery. Mol Med Today.
4 Russell S.J., Peng K.W. (2007). Viruses as anticancer drugs. Trends Pharmacol Sci.
5 Condreay J.P., Kost T.A. (2007). Baculovirus expression vectors for insect and mammalian cells. Curr Drug Targets.
6 Raty, J.K., Baculovirus surface modifications for enhanced gene delivery and biodistribution imaging, in Kuopio Univesity Hispotal2006, Kuopio Univesity. p. 86.
7 Kost T.A., Condreay J.P. (2002). Recombinant baculoviruses as mammalian cell gene-delivery vectors. Trends Biotechnol.
8 Raty J.K., Airenne K.J., Marttila A.T., Marjomaki V., Hytonen V.P., Lehtolainen P., Laitinen O.H., Mahonen A.J., Kulomaa M.S., Yla-Herttuala S. (2004). Enhanced gene delivery by avidin-displaying baculovirus. Mol Ther.
9 Raty J.K., Liimatainen T., Wirth T., Airenne K.J., Ihalainen T.O., Huhtala T., Hamerlynck E., Vihinen-Ranta M., Narvanen A., Yla-Herttuala S., Hakumaki J.M. (2006). Magnetic resonance imaging of viral particle biodistribution in vivo. Gene Ther.
10 Josephson L., Perez J.M., Weissleder R. (2001). Magnetic nanosensors for the detection of oligonucleotide sequences. Angew. Chem. Int. Ed. Engl.
11 Bulte J.W., Brooks R.A., Moskowitz B.M., Bryant L.H., Frank J.A. (1998). T1 and T2 relaxometry of monocrystalline iron oxide nanoparticles (MION-46L): theory and experiment. Acad Radiol.
12 Serebriiskii I.G., Golemis E.A. (2000). Uses of lacZ to study gene function: evaluation of beta-galactosidase assays employed in the yeast two-hybrid system. Anal Biochem.